# ^111^In-Benzyl-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Z_HER2:342_

Chemical name: | ^111^In-Benzyl-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Z_HER2:342_
Abbreviated name: | ^111^In-Benzyl-DOTA-Z_HER2:342_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | SPECT
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A was constructed (17). Affibody molecules exhibit high binding affinity (K_d_) to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. Z_HER2:342_ was labeled with ^111^In via isothiocyanate-benzyl-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Z_HER2:342_ to form ^111^In-benzyl-DOTA-Z_HER2:342_ for single-photon emission computed tomography (SPECT) imaging in nude mice bearing human tumors (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+affibody)]

Isothiocyanate-benzyl-DOTA and Z_HER2:342_ (3:1 molar ratio) were incubated in sodium borate buffer (pH 9) at 37ºC for 20 h (18). Benzyl-DOTA-Z_HER2:342_ was isolated from the incubation mixture with a NAP-5 column. High-performance liquid chromatography-mass spectometry analysis revealed that 59% of benzyl-DOTA-Z_HER2:342_ contained one DOTA moiety, 26% had two DOTA, and 15% was unconjugated. Benzyl-DOTA-Z_HER2:342_ (500 μg) was mixed with 40 MBq (1.08 mCi) ^111^InCl_3_. The mixture was incubated at 60ºC for 15 min with a labeling efficiency of >97%. ^111^In-Benzyl-DOTA-Z_HER2:342_ was purified with NAP-5 chromatography with a radiochemical purity of >98%. ^111^In-Benzyl-DOTA-Z_HER2:342_ was stable in phosphate-buffered saline and ethylenediamine tetraacetic acid buffer with >95% of ^111^In associated with benzyl-DOTA-Z_HER2:342_ after 3 h of incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20in%20vitro)]

Orlova et al. (18) performed in vitro binding specificity tests, which showed that binding of ^111^In-benzyl-DOTA-Z_HER2:342_ to SKOV-3 cells expressing HER2 was mediated by the receptors because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^111^In-benzyl-DOTA-Z_HER2:342_. The cell-bound radioactivity remained at 38–40% of the initially bound activity for up to 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20rodentia)]

Orlova et al. (18) performed biodistribution studies of ^111^In-benzyl-DOTA-Z_HER2:342_ (0.05 MBq (1.35 μCi)) in nude mice (n = 4/group) bearing LS174T xenografts. The initial tracer accumulation in the LS174T tumors was 4.4% injected dose per gram (ID/g) at 4 h after injection. The organ with the highest radioactivity at 4 h was the kidney (232% ID/g), followed by the liver (3% ID/g). The radioactivity level in tumors was higher than in other organs and tissues (except the kidney). Blood level was ~0.2% ID/g at 4 h with a tumor/blood ratio of 22. Pre-administration of excess Z_HER2:342_ decreased tumor accumulation by 7.7-fold at 4 h after injection. Some inhibition was observed in the lung, liver, and spleen. Positron emission tomography analysis was performed in nude mice bearing the SKOV-3 tumors after intravenous injection of 3 MBq (81 μCi) ^111^In-benzyl-DOTA-Z_HER2:342_. Tumors were clearly visualized at 4 h along with the kidneys. The tumor/muscle, tumor/liver, and tumor/kidney ratios were 33.0, 3.3, and 0.2, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Orlova A., Tran T., Widstrom C., Engfeldt T., Eriksson Karlstrom A., Tolmachev V. (2007). Pre-clinical evaluation of [111In]-benzyl-DOTA-Z(HER2:342), a potential agent for imaging of HER2 expression in malignant tumors. Int J Mol Med.